# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu
Abbreviated name: | ^64^Cu-NO2A-(GSG)-KCCYSL
Synonym:
Agent category: | Peptide
Target: | Epidermal growth factor receptor-2 (EGFR-2, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells, such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A setapeptide sequence consisting of Lys-Cys-Cys-Tyr-Ser-Leu (KCCYSL) was identified using phage display screening to bind specifically to the extracellular domain of HER2 (17). ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7-tris-acetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^111^In-DOTA-(GSG)-KCCYSL (http://www.ncbi.nlm.nih.gov/books/NBK23014/)) was evaluated in nude mice bearing human breast tumor xenografts for single-photon emission computed tomography imaging (18). For positron emission tomography (PET), Kumar et al. (19) prepared ^64^Cu-1,4,7-triazacyclononane-1,4-diacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^64^Cu-NO2A-(GSG)-KCCYSL) for imaging of HER2 expression in breast tumors.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20synthesis)]

GSG-KCCYSL peptides were prepared with solid-phase peptide synthesis (19). The metal chelator NOTA was coupled to the amino terminus of GSG-KCCYSL with solid-phase synthesis. NO2A-(GSG)-KCCYSL was purified with high-performance liquid chromatography (HPLC). The chemical purity of NO2A-(GSG)-KCCYSL was 98%. NO2A-(GSG)-KCCYSL (37.6 nmol) was mixed with 29.6 MBq (0.80 mCi) ^64^Cu in ammonium acetate (pH 6.4) and incubated for 60 min at 75°C. ^64^Cu-NO2A-(GSG)-KCCYSL was purified with HPLC, with >98% radiochemical purity and 57% labeling yield. The specific activity of ^64^Cu-NO2A-(GSG)-KCCYSL was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20in%20vitro)]

Kumar et al. (19) performed in vitro binding assays of ^64^Cu-NO2A-(GSG)-KCCYSL binding to human MDA-MB-435 breast carcinoma cells that express HER2 receptors. ^nat^Cu-NO2A-(GSG)-KCCYSL exhibited a IC_50_ value of 44 ± 7 nM (n = 3). ^64^Cu-NO2A-(GSG)-KCCYSL accumulated in MDA-MB-435 cells in a time-dependent manner at 37°C with a plateau at 45 min, whereas little radioactivity was observed in normal human mammary epithelial cells (184A1) that express low levels of HER2 receptors. ^64^Cu-NO2A-(GSG)-KCCYSL was stable in mouse serum at 37°C after up to 2 h of incubation with some degradation at 4–24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20rodentia)]

Kumar et al. (19) performed ex vivo biodistribution studies with 0.185 MBq (5 μCi) ^64^Cu-NO2A-(GSG)-KCCYSL in SCID mice (n = 3/group) bearing MDA-MB-435 xenografts at 0.5, 1, 2, and 4 h after injection. The tumor accumulation of radioactivity at 0.5 h after injection was 0.78 ± 0.03% injected dose/gram (ID/g) and decreased to 0.43 ± 0.02% ID/g at 4 h. High accumulation levels were observed in the kidneys (4.23 ± 1.00% ID/g), lung (0.49 ± 0.07% ID/g), and liver (0.48 ± 0.05% ID/g) at 2 h after injection. The tumor/blood, tumor/muscle, and tumor/liver ratios were 7.6, 10.7, and 1.3 at 2 h after injection, respectively. Pretreatment (10 min) with ^nat^Cu-NO2A-(GSG)-KCCYSL (76 nmol/mouse) inhibited the tumor radioactivity by 50% at 2 h after injection. Little inhibition was observed in the normal tissues. In comparison, ^64^Cu-NO2A-(GSG)-KCCYSL exhibited lower retention in the liver and higher tumor/nontarget tissue ratios than ^64^Cu-DO3A-(GSG)-KCCYSL, which exhibited liver accumulation of 1.68 ± 0.42% ID/g and tumor/blood, tumor/muscle, and tumor/liver ratios of 2.7, 9.0, and 0.3 at 2 h after injection, respectively.

PET analysis was performed in SCID mice (the number of mice was not reported) bearing the MDA-MB-435 tumors at 2 h after injection of 12 MBq (0.32 mCi) ^64^Cu-NO2A-(GSG)-KCCYSL (19). The tumors were clearly visualized along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20human)]

No publication is currently available.

## NIH support

P50 CA103130-01, IR21 CA137239-01A1, 2 R01 CA093375

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Karasseva N.G., Glinsky V.V., Chen N.X., Komatireddy R., Quinn T.P. (2002). Identification and characterization of peptides that bind human ErbB-2 selected from a bacteriophage display library. J Protein Chem.
18 Deutscher S.L., Figueroa S.D., Kumar S.R. (2009). In-labeled KCCYSL peptide as an imaging probe for ErbB-2-expressing ovarian carcinomas. J Labelled Comp Radiopharm.
19 Kumar S.R., Gallazzi F.A., Ferdani R., Anderson C.J., Quinn T.P., Deutscher S.L. (2010). In vitro and in vivo evaluation of Cu-radiolabeled KCCYSL peptides for targeting epidermal growth factor receptor-2 in breast carcinomas. Cancer Biother Radiopharm.